# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 diabody

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 diabody
Abbreviated name: | ^111^In-DOTA-T84.66 diabody
Synonym:
Agent category: | Antibody fragment
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT)
Source of signal\contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+diabody)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory conditions such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in the serum (5). CEA expression is observed in patients with various carcinomas of the colon, lungs, thyroid, uterus, ovaries, pancreas, and medullary thyroid (6). Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (7, 8). ^99m^Tc-Arcitumomab, a murine anti-CEA mAb Fab’ fragment, was developed for use in single-photon emission computed tomography (SPECT) imaging of CEA expression.

Single-chain variable fragments (scFvs) of antibodies with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (9). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass = 55 kDa) has been evaluated for targeting in several tumor antigen systems and has demonstrated rapid tumor localization and high-contrast imaging (9, 10). In particular, murine/human chimeric anti-CEA T84.66 antibodies, which retain excellent CEA-binding properties (dissociation constant = 0.01–0.6 nM) (11-13), were developed as CEA imaging agents. A T84.66 diabody was conjugated with 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) and radiolabeled with ^111^In for localization of CEA-positive tumors in mice (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+diabody+and%20synthesis)]

A mixture of recombinant T84.66 diabody and N-hydroxysuccinimidyl-DOTA in a 1:1,000 molar ratio was incubated at 4°C for 18 h (14, 15). The DOTA/diabody ratio was determined to be 0.5. The DOTA-diabody (~7.3 nmol) was incubated with 48.1 MBq (1.3 mCi) of ^111^InCl_3_ in 0.25 NH_4_OAc at 43°C for 1 h. ^111^In-DOTA-T84.66 diabody was isolated with gel filtration through a column with a radiochemical purity of >98%. The overall radiochemical yields were 67–100%. The specific activity was 2.9–6.6 GBq/μmol (77.8–177.8 mCi/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+diabody+and%20in%20vitro)]

Radioimmunoreactivity of ^111^In-DOTA-T84.66 diabody for N-A3 (a recombinant CEA fragment) was determined with size-exclusion high-performance liquid chromatography analysis to be >95% (14). The affinity constant of DOTA-T84.66 diabody was not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+diabody+and%20rodentia)]

Yazaki et al. (14) performed biodistribution studies of ^111^In-DOTA-T84.66 diabody in nude mice (n = 5 mice/group) with the use of an LS174T subcutaneous xenograft model. Data were obtained at 2, 4, 6, 12, and 24 h after injection. ^111^In-DOTA-T84.66 diabody had a rapid blood clearance, resulting in very low activity in the blood at 2, 4, and 12 h (2.70 ± 0.38%, 0.64 ± 0.14%, and 0.11 ± 0.03% injected dose (ID)/g, respectively). The blood clearance pattern exhibited a two-phase model with a half-life of 0.43 h during the distribution phase and a half-life of 3.04 h during the elimination phase. The tracer accumulation in the CEA-expressing tumor was 12.5 ± 1.0% ID/g at 2 h, 13.3 ± 2.1% ID/g at 6 h, 12.3 ± 3.1% ID/g at 12 h, and 7.7 ± 1.0% ID/g at 24 h. The kidney had the highest accumulation with a peak of 183.5 ± 21.0% ID/g at 6 h. All other major organs exhibited lower levels of radioactivity than the tumor. The tumor/blood ratio increased significantly over time (4.7 ± 0.4, 19.4 ± 1.6, 39.5 ± 3.4, and 196 ± 11.1 at 2, 4, 6, and 24 h after injection, respectively). The tumor/liver ratio remained steady over time (2.2–3.5). Pre-administration of an oral dose of 100 mg D-lysine 30 min before ^111^In-DOTA-T84.66 diabody resulted in a 59% reduction of the renal accumulation at 6 h. However, there was a related 31% reduction of tumor accumulation. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+diabody+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+diabody+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+diabody+and%20human)]

No publication is currently available.

## NIH Support

P01 CA43904, CA33572

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab1999, Immunomedics, Inc. p. 1-15.
7 Kenanova V., Wu A.M. (2006). Tailoring antibodies for radionuclide delivery. Expert Opin Drug Deliv.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
10 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
11 Fagerstam L.G., Frostell-Karlsson A., Karlsson R., Persson B., Ronnberg I. (1992). Biospecific interaction analysis using surface plasmon resonance detection applied to kinetic, binding site and concentration analysis. J Chromatogr.
12 Hefta L.J., Neumaier M., Shively J.E. (1998). Kinetic and affinity constants of epitope specific anti-carcinoembryonic antigen (CEA) monoclonal antibodies for CEA and engineered CEA domain constructs. Immunotechnology.
13 Williams L.E., Wu A.M., Yazaki P.J., Liu A., Raubitschek A.A., Shively J.E., Wong J.Y. (2001). Numerical selection of optimal tumor imaging agents with application to engineered antibodies. Cancer Biother Radiopharm.
14 Yazaki P.J., Wu A.M., Tsai S.W., Williams L.E., Ikler D.N., Wong J.Y., Shively J.E., Raubitschek A.A. (2001). Tumor targeting of radiometal labeled anti-CEA recombinant T84.66 diabody and t84.66 minibody: comparison to radioiodinated fragments. Bioconjug Chem.
15 Yazaki P.J., Shively L., Clark C., Cheung C.W., Le W., Szpikowska B., Shively J.E., Raubitschek A.A., Wu A.M. (2001). Mammalian expression and hollow fiber bioreactor production of recombinant anti-CEA diabody and minibody for clinical applications. J Immunol Methods.